# Cy5.5-Arg-Arg-Arg-Arg-crosslinked iron oxide nanoparticle

Chemical name: | Cy5.5-Arg-Arg-Arg-Arg-crosslinked iron oxide nanoparticle
Abbreviated name: | Cy5.5-R4-SC-CLIO
Synonym:
Agent category: | Peptide
Target: | Proteases
Target category: | Enzyme
Method of detection: | Multimodality: Optical, Near-infrared (NIR) fluorescence imaging and magnetic resonance imaging (MRI)
Source of signal: | Cy5.5 and iron oxides
Activation: | Yes
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIRF%5BAll%20Fields%5D%20AND%20clio%5BAll%20Fields%5D)]

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets in vitro and in small animals (1, 2). Near-infrared (NIR) fluorescence (700-900 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background because of reduced scattering compared to visible fluorescence detection. They also have high sensitivity resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alterative to radionuclide imaging in vitro and in small animals.

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules. Water comprises >80% of most soft tissues. The contrast of proton MRI depends mainly on the density of nuclear (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires development of contrast agents. Most of the contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T-2* is the spin-spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (3).

Superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxide particles are coated with a protective layer of dextran or other polysaccharide (3). These particles have large combined magnetic moments or spins, which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into the reticuloendothelial system (RES) is by endocytosis or phagocytosis. SPIO particles are taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A chimeric nanoparticles probe was constructed with a Cy5.5-R4 (L-Arg-Arg-Arg-Arg peptide) and cross-linked iron oxide (CLIO) nanoparticles to form Cy5.5-R4-SC-CLIO (4, 5). The Cy5.5-R4 part of the probe is activated by protease activity in the local environment, whereas the CLIO part is to provide spatial/anatomic information.

### Related Resource Links:

- Chapters in MICAD (MMP (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=matrix+metalloproteinases+AND+micad%5Bbook%5D))
- Gene information in NCBI (MMP2 (http://www.ncbi.nlm.nih.gov/gene/4313), MMP9 (http://www.ncbi.nlm.nih.gov/gene/4318))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MMP2 (http://omim.org/entry/120360), MMP9 (http://omim.org/entry/120361))
- Clinical trials (MMP (http://www.clinicaltrials.gov/ct2/results?term=matrix+metalloproteinases))
- Drug information in FDA (MMP (http://google2.fda.gov/search?q=matrix+metalloproteinases+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIRF%5BAll%20Fields%5D%20AND%20CLIO%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

Aminated CLIO consists of a core of SPIO, a cross-linked coating of dextran with amino groups, which was reacted with succinimidyl iodoacetate followed by R4 to produce R4-SC-CLIO (4, 5). Cy5.5 was attached to R4-SC-CLIO using N-hydroxylsuccinimidyl (NHS) ester of Cy5.5 to yield Cy5.5-R4-SC-CLIO. Unreacted Cy5.5-NHS dye was removed using a PD-10 column. The sizes of the Cy5.5-R4-SC-CLIO nanoparticles were determined by laser light scattering to be 62 ± 7 nm. There were 15.5 R4 peptides and 1.79 Cy5.5 fluorophores per nanoparticle. The R1 and R2 relaxivities were 29.9 and 92.5 s^-1^mM^-1^, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIRF%5BAll%20Fields%5D%20AND%20CLIO%5BAll%20Fields%5D%20AND%20in%20vitro)]

Incubation (for 200 min) of Cy5.5-R4-SC-CLIO (25 μg Fe/ml) with cathepsin B (1.6 μg/ml) or trypsin (10 μg/ml) increased the NIR fluorescent intensity 27.4-fold by cleaving the L-Arg residues in the probe (4). Cy3.5-r4-SC-CLIO or Cy5.5-r4-SS-CLIO with D-Arg residues showed no increase in NIR fluorescence in the presence of the enzymes.

A mixture of Cy5.5-R4-SC-CLIO and Cy3.5-r4-SC-CLIO was incubated with different numbers of murine macrophages (5 X 10^6^, 10 X 10^6^, and 15 X 10^6^ cells/0.1 ml) in the presence or absence of cathepsin inhibitors (5). The Cy5.5 and Cy3.5 fluorescence in the cells was measured after 6 h of incubation. Increasing numbers of cells were associated with increases in fluorescence for both fluorophores, indicating that both probes were internalized by macrophages. Cy5.5 fluorescence increase was blocked by cathepsin inhibitors, while Cy3.5 fluorescence was not. This is because Cy5.5-R4-SC-CLIO was activated by macrophages, and Cy3.5-r4-SC-CLIO was not.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIRF%5BAll%20Fields%5D%20AND%20CLIO%5BAll%20Fields%5D%20AND%20rodentia)]

To study the feasibility of using Cy5.5-R4-SC-CLIO nanoparticles as a combined optical and MR contrast agent, mice were injected with 5.1 mg/kg (2 nmol) of Cy5.5-R4-SC-CLIO (4). After 18 h, MR and NIR fluorescence images were obtained from excised tissues. Uptake of Cy5.5-R4-SC-CLIO was evident in the spleen and lung from a loss of T2 signal as compared with a control mouse. There was good uptake in the liver, spleen, and kidneys, as measured by Cy5.5 signal. Whole-body imaging of a mouse that received an injection of Cy5.5-R4-SC-CLIO showed a loss of T2 signal from the axillary and brachial nodes by MR imaging. Reflectance imaging also showed Cy5.5 fluorescence signal from these nodes. These studies suggested a role of macrophages in the RES of the liver, spleen, and lung to accumulate the probe. Increased NIR fluorescence signal may be because of high concentrations of proteases in macrophages in these organs.

Mice received injections of a mixture of Cy5.5-R4-SC-CLIO and Cy3.5-r4-SC-CLIO, and selected tissues were excised 24 h after injection for NIR fluorescence measurement (5). The organ with the highest Cy5.5-to-Cy3.5 NIR fluorescence ratio was the liver (59.4), followed by the spleen (26.6), lung (25.5), kidneys (25.0), and muscle (17.0). The injection mixture had a ratio of 8.9. The increase in the ratio over the injection mixture indicates the activation of the Cy5.5 probe by cathepsin in these organs and not the activation of the Cy3.5-r4-SC-CLIO probe. Cy5.5-R4-SC-CLIO is capable of localizing its position through its magnetic properties (CLIO), providing functional information (protease activity) by optical imaging technology (Cy5.5-R4).

When CLIO is phagocytized, the exchangeable water is excluded; therefore, there is a loss of MRI signal. The NIR fluorescence signal increased because of hydrolysis by macrophage proteases in the nodes. Cy5.5-R4-SC-CLIO has a T1/T2 MRI signal in an aqueous environment and a low Cy5.5 fluorescence signal. When proteases cleave the R-R bond to form Cy5.5-RR and RR-SC-CLIO, NIR fluorescence is increased from Cy5.5-RR as compared with Cy5.5-R4-SC-CLIO, either in solution or inside the macrophages. The RR-SC-CLIO MRI signal is decreased if RR-SC-CLIO is formed inside the macrophages. The Cy5.5-R4-SC-CLIO MRI signal is also decreased if it is engulfed by the macrophages without hydrolysis, and in this case, little change in NIR fluorescence signals, as shown by protease inhibition.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIRF%5BAll%20Fields%5D%20AND%20CLIO%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIRF%20AND%20CLIO%20and%20%28primates%20not%20humans%29)]

No publication is currently available

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIRF%20AND%20CLIO%20and%20humans)]

No publication is currently available.

## NIH Support

P01 CA69246, P50 CA86355, R24 CA92782, R33 CA88365

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
4 Josephson L., Kircher M.F., Mahmood U., Tang Y., Weissleder R. (2002). Near-infrared fluorescent nanoparticles as combined MR/optical imaging probes. Bioconjug Chem.
5 Kircher M.F., Josephson L., Weissleder R. (2002). Ratio imaging of enzyme activity using dual wavelength optical reporters. Mol Imaging.